# Radioiodinated anti-CEA monoclonal antibody NP-4 F(ab´)_2_ fragment

Chemical name: | Radioiodinated anti-CEA monoclonal antibody NP-4 F(ab´)_2_ fragment
Abbreviated name: | ^123^I/^131^I/^125^I-NP-4 F(ab´)_2_
Synonym: | ^131^I-NP-4 F(ab´)_2_ anti-CEA monoclonal antibody, ^125^I-NP-4 F(ab´)_2_ anti-CEA monoclonal antibody, ^123^I-NP-4 F(ab´)_2_ anti-CEA monoclonal antibody, ^131^I-NP-4 F(ab´)_2_ MAb, ^125^I-NP-4 F(ab´)_2_ MAb, ^123^I-NP-4 F(ab´)_2_ MAb
Agent Category: | Antibody F(ab´)_2_ fragment
Target: | Carcinoembryonic antigen (CEA)
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^131^I, ^123^I, ^125^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20F%28ab%27%292%20OR%20iodine-131-labeled%20anti-CEA%20monoclonal%20antibody%20NP-4%20F%28ab%27%292%20OR%20NP-4%20F%28ab%27%292%29)]

Radioiodinated anti-carcinoembryonic antigen (CEA) monoclonal antibody (MAb) NP-4 F(ab´)_2_ fragment (^123^I/^131^I/^125^I-NP-4 F(ab´)_2_), which is formed by the conjugation of radioiodine with a murine anti-CEA MAb F(ab´)_2_ fragment, can be used for imaging and therapy of CEA-expressing cancers (1, 2). ^125^I has a relatively long physical half-life (t_½_) of 60 days and a gamma energy that makes it suitable for imaging only in small animals. ^131^I has a physical half-life (t_½_) of 8.02 days with a gamma energy that is high but acceptable for in vivo imaging. ^123^I, another radioiodine, has better physical properties for single-photon emission computed tomography (SPECT) and planar gamma imaging in humans.

CEA was first identified from extracts of human adenocarcinoma of the colon (3). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas, particularly of the gastrointestinal tract, as well as in fetal gastrointestinal tissues and in certain inflammatory states, such as inflammatory bowel disease (4, 5). CEA, which exhibits extensive heterogeneity in its physicochemical and immunologic properties (2, 3), has a molecular mass of 200 kDa and can be shed and detected in the serum (2). It has been used as a serum marker for monitoring disease status in patients who have various CEA-secreting tumors (gastrointestinal, lung, medullary, thyroid, uterine, ovarian, and bladder carcinomas). Other cross-reactive, but genetically distinct, CEA variants have been identified, including nonspecific cross-reactive antigen (NCA) and meconium antigen (MA) (6).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (4). Primus et al. (2) studied the immunologic heterogeneity of CEA by use of four MAbs to differentiate the antigenic sites on colonic cancer CEA. They classified the MAbs into three general classes based on their reactivity with CEA, NCA, and MA. The class I antibody, NP-1, had high affinity for CEA and MA but low affinity for NCA. The class II antibodies, NP-2 and NP-3, had moderate affinities for CEA and MA. The class III antibody, NP-4, appeared to recognize determinants unique to CEA and had no affinity for NCA or MA. Because of this specificity, NP-4 MAb has been labeled with radionuclides for CEA tumor imaging and therapy (7). Intact NP-4 MAb can be covalently linked to ^131^I, ^123^I, or ^125^I by direct radioiodination with Na^131^I, Na^123^I, or Na^125^I, using an appropriate oxidizing agent. Because of differences in their radiation physical properties, ^131^I can be used for both therapy and imaging, ^123^I is used only for imaging, and ^125^I is used mainly for in vitro studies. The in vivo pharmacokinetics of intact radiolabeled immunoglobulin G (IgG) in humans are characterized by high liver uptake and slow blood elimination. Therefore, the intact radiolabeled NP-4 MAb is generally not ideal for imaging. Smaller radiolabeled MAb fragments such as Fob or F(ab´)_2_ may have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Covell et al. (8) reported that the percentages of total body catabolism of an i.v.-administered ^131^I-labeled MAb and its fragments by the kidney were 1.7% (intact IgG), 50.3% (F(ab´)_2_), and 73.4% (Fab´).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20F%28ab%27%292%20OR%20iodine-131-labeled%20anti-CEA%20monoclonal%20antibody%20NP-4%20F%28ab%27%292%20OR%20NP-4%20F%28ab%27%292%29%20AND%20synthesis)]

NP-4 MAb is an IgG_1_ subtype and has a CEA affinity in the range of 10^8^ M^–1^ (2, 5). NP-4 MAb was initially produced by Primus et al. (2) in 1983; they used the hybridoma technique and CEA isolated from liver metastases of a colonic adenocarcinoma. The NP-4 MAb was produced in mice and purified from ascites fluid by protein A and ion-exchange column chromatography at 4 °C (9). Sharkey et al. (10-13) and Blumenthal et al. (2) first reported the preparation of NP-4 F(ab´)_2_ by pepsin digestion in 0.1 M sodium citrate buffer, pH 3.5, at 37 °C for 45-90 min. The reaction was stopped by increasing the pH to 7.0. The preparation was desalted on a fractogel column. Isolation was done by either protein A or ion-exchange chromatography. The final purity and identity were confirmed by immunoelectrophoresis, sodium dodecyl sulfate gel electrophoresis, and size-exclusion high-performance liquid chromatography. Direct radioiodination of the NP-4 F(ab´)_2_ with ^131^I was performed by the chloramine-T method using a ratio of 0.06 mg of F(ab´)_2_ per mCi of ^131^I. Unbound radioactive iodine was separated from ^131^I-NP-4 F(ab´)_2_ by gel filtration. The specific activity obtained was 444-555 MBq/mg (12-15 mCi/mg), or 20.4-55.5 GBq/µmol (1.2-1.5 Ci/µmol) based on a molecular weight of 100,000 for the F(ab´)_2_ fragment. The radiochemical purity was 95-98%, and there was <1% aggregated antibody. Goldenberg et al. (14) achieved similar labeling efficiency with ^123^I. Juweid et al. (15) used the IodoGen method for ^131^I radioiodination and obtained a similar specific activity of 444-592 MBq/mg (12-16 mCi/mg), or 20.4-59.2 GBq/µmol (1.2-1.6 Ci/µmol). Radiochemical purity was >98%, and there was <7% aggregated antibody.

## In Vitro Studies: Testing in Cells and Tissues

Primus et al. (2) first reported the production of NP-4 anti-CEA MAb. Using a competitive radioimmunoassay method, they obtained an affinity constant (K) for CEA of 8.9 × 10^8^ M^–1^. NP-4 MAb did not appear to bind to NCA or MA. Sharkey et al. (10-13) and Blumenthal et al. (2) determined the immunoreactivity of ^131^I-NP-4 F(ab´)_2_ by affinity chromatography on a CEA immunoabsorbent. The ^131^I-NP-4 F(ab´)_2_ prepared by the chloramine-T method had 75-85% binding. Juweid et al. (15) found that the ^131^I-NP-4 F(ab´)_2_ prepared by the IodoGen method had >70% binding.

## Animal Studies

### Rodents

Sharkey et al. (11) studied the biodistribution of ^131^I-NP-4 F(ab´)_2_ and the intact ^131^I-NP-4 MAb in athymic nude mice bearing the CEA-producing human colorectal cancer, GW-39. ^131^I-NP-4 F(ab´)_2_ tumor uptake was highest (10-20% of injected dose (ID)/g) on days 1 and 2. Tumor accretion of ^131^I-NP-4 F(ab´)_2_ was highest (4-5% ID/g) at 6 h after injection and remained constant from day 1 to day 3. In comparison, maximum tumor localization of ^131^I-NP-4 MAb occurred on day 3 and reached about 30% ID/g. On day 1, the ^131^I-NP-4 F(ab´)_2_ tumor/nontumor ratios (n = 4-6) were 2.0 ± 0.7 (tumor/blood), 3.2 ± 0.8 (tumor/lung), 7.1 ± 1.6 (tumor/liver), and 3.7 ± 1.2 (tumor/kidney). For the intact ^131^I-NP-4 MAb, these ratios were 0.9 ± 0.3 (tumor/blood), 2.1 ± 0.8 (tumor/lung), 3.8 ± 1.3 (tumor/liver), and 2.5 ± 0.9 (tumor/kidney). On day 3, the ^131^I-NP-4 F(ab´)_2_ tumor/nontumor ratios were increased to 9.1 ± 3.0 (tumor/blood), 14.5 ± 4.8 (tumor/lung), 26.6 ± 6.6 (tumor/liver), and 14.2 ± 3.6 (tumor/kidney). For the ^131^I-NP-4 MAb, these ratios were 2.2 ± 0.8 (tumor/blood), 5.3 ± 1.8 (tumor/lung), 8.6 ± 2.8 (tumor liver), and 7.1 ± 2.7 (tumor/kidney).

In another study, Sharkey et al. (12) reported radiation dose estimates of ^131^I-NP-4 F(ab´)_2_ in GW-39 tumor-bearing nude mice. The estimates were based on a dose of 50.69 MBq (1.37 mCi), which would give a 50-Gy (5,000 rads) radiation absorbed dose to the tumor. The doses for the blood, kidney, liver, lung, and spleen were 8.54, 7.01, 3.74, 8.09, and 3.86 Gy (854, 701, 374, 809, and 386 rads), respectively.

Blumenthal et al. (16) evaluated the targeting of ^131^I-NP-4 F(ab´)_2_ to micrometastases in a micrometastatic lung model. Intravenous injection of GW-39 tumor cells into nude mice resulted in 40-80 tumor nodules (50-200 μm in diameter within 7 days) throughout the lungs. Each mouse received 370 kBq (10 μCi)/6 μg of MAb. The radioactivities (% ID/g; n = 5) at 24 h for the lung tumor nodules, s.c. tumor, and blood were 2.3 ± 0.5, 6.3 ± 0.7, and 3.8 ± 0.7, respectively. On the basis of a highest possible dose resulting in no animal death (maximum tolerated dose) of 44.4 MBq (1.2 mCi), the radiation absorbed doses were 5.5 (lung tumor nodules), 22.57 (s.c. tumor), and 8.95 Gy (blood) (550, 2,257, and 895 rads, respectively). Fand et al. (17) also studied tumor metastases in the lung and liver, using whole-body macroautoradiography. Each mouse received 555 kBq (15 μCi) of ^125^I-NP-4 F(ab´)_2_. The densitometrically derived tumor/nontumor ratios on day 1 for the metastatic lung tumor were 1.9 (tumor/blood), 4.3 (tumor/liver), 2.8 (tumor/kidney), and 2.8 (tumor/lung). On day 3, all of these ratios were 11. For the metastatic liver tumor on day 1, the ratios were 6.3 (tumor/blood), 14.3 (tumor/liver), 9.5 (tumor/kidney), and 9.5 (tumor/lung), and all of these ratios increased to 57 on day 3.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20F%28ab%27%292%20OR%20iodine-131-labeled%20anti-CEA%20monoclonal%20antibody%20NP-4%20F%28ab%27%292%20OR%20NP-4%20F%28ab%27%292%29%20AND%20%28dog%20OR%20rabbit)]

Sharkey et al. (10) studied the biodistribution of ^131^I-NP-4 F(ab´)_2_ and intact ^131^I-NP-4 in hamsters bearing the human colorectal carcinoma GW-39 in the hind leg muscle. Each tumor-bearing hamster received intracardiac injections containing 5,550-7,400 kBq (150-200 µCi)/10-15 µg of ^131^I-NP-4 F(ab´)_2_ or ^131^I-NP-4. Both ^131^I-NP-4 F(ab´)_2_ and ^131^I-NP-4 showed a preferential localization for GW-39. ^131^I-NP-4 F(ab´)_2_ was cleared from the blood and normal tissues more rapidly than the intact ^131^I-NP-4. By day 3, there was 2.5 times less radioactivity in the tumor with ^131^I-NP-4 F(ab´)_2_ compared with the intact ^131^I-NP-4. In the blood, there was 4 times less radioactivity with ^131^I-NP-4 F(ab´)_2_ compared with ^131^I-NP-4.

Blumenthal et al. (13) evaluated the in vivo uptake, therapeutic potential, and host toxicity of ^131^I-NP-4 F(ab´)_2_ in GW-39 tumors grown in hamster check pouches. The animals received i.p. injections containing 3.7 MBq (0.1 mCi)/6 μg (MAb) of either ^131^I-NP-4 F(ab´)_2_ or ^131^I-NP-4. The tumor radioactivity concentrations (% ID/g; n = 10-18) for ^131^I-NP-4 F(ab´)_2_ on days 1 and 2 were 0.92 ± 0.44 and 1.24 ± 0.46, respectively. The tumor radioactivity concentrations (% ID/g; n = 10-21) for ^131^I-NP-4 on days 1 and 3 were 1.20 ± 2.1 and 5.57 ± 0.56, respectively. The radioactivity concentrations (% ID/g; n = 5-9) on day 1 for ^131^I-NP-4 F(ab´)_2_ were 0.99 ± 0.23 (blood), 0.51 ± 0.22 (lungs), 0.53 ± 0.18 (kidney), 0.28 ± 0.13 (spleen), and 0.27 ± 0.09 (liver). On day 3, these values decreased to 0.11 ± 0.04 (blood), 0.05 ± 0.02 (lungs), 0.07 ± 0.02 (kidney), 0.03 ± 0.01 (spleen), and 0.03 ± 0.01 (liver). For ^131^I-NP-4, the % ID/g values in the same organs on day 1 were 2.48 ± 0.09 (blood), 1.05 ± 0.06 (lungs), 0.82 ± 0.1 (kidney), 0.66 ± 0.03 (spleen), and 0.83 ± 0.02 (liver), On day 3, these values decreased to 1.34 ± 0.12 (blood), 0.79 ± 0.09 (lungs), 0.58 ± 0.06 (kidney), 0.36 ± 0.03 (spleen), and 0.47 ± 0.03 (kidney), The ^131^I-NP-4 F(ab´)_2_ cumulative absorbed doses were 0.11 (tumor), 0.014 (liver), 0.01 (spleen), 0.02 (kidney), and 0.018 (lung) Gy/MBq (420, 52, 36, 77, and 68 rads/mCi, respectively).

### Non-Human Primates

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20F%28ab%27%292%20OR%20iodine-131-labeled%20anti-CEA%20monoclonal%20antibody%20NP-4%20F%28ab%27%292%20OR%20NP-4%20F%28ab%27%292%29%20AND%20%28primate%20NOT%20h)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28131I-NP-4%20F%28ab%27%292%20OR%20iodine-131-labeled%20anti-CEA%20monoclonal%20antibody%20NP-4%20F%28ab%27%292%20OR%20NP-4%20F%28ab%27%292%29%20AND%20human)]

Murray et al. (18) conducted a tumor localization study of ^131^I-NP-4 F(ab´)_2_ in 5 patients with either liver metastases from colorectal cancer or intact primary tumors. Patients received both ^131^I-NP-4 F(ab´)_2_ (1 mg of F(ab´)_2_ labeled with 10 mCi of ^131^I) and intact ^125^I-NP-4 MAb (1 mg of NP-4 labeled with 2 mCi of ^125^I) in a mixture. Gamma imaging and autoradiography of tissues from biopsies were used to determine radioactivity localization. For ^131^I-NP-4 F(ab´)_2_, the pharmacokinetic parameters plasma half-life (t_½_), volume of distribution, plasma clearance, and 48-h urinary excretion were 29.0 ± 3.2 h, 3.8 ± 0.4 liters, 1.5 ± 0.2 ml/kg/min, and 50.2 ± 5.0%, respectively. For ^125^I-NP-4 MAb, these parameters were 43.2 ± 7.3 h, 3.3 ± 0.2 liters, 0.9 ± 0.2 ml/kg/min, and 56.7 ± 4.7%, respectively. The tumor radioactivity uptakes (% ID/kg) of ^131^I-NP-4 F(ab´)_2_ and ^125^I-NP-4 MAb were 2.0 ± 0.57 and 2.6 ± 0.94, respectively. The ^131^I-NP-4 F(ab´)_2_ tumor/normal tissue ratios were 6.0 ± 2.1 (tumor/liver), 0.83 ± 0.21 (tumor/blood), and 7.6 ± 2.3 (tumor/other tissue). For ^125^I-NP-4 MAb, these ratios were 3.1 ± 0.61 (tumor/liver), 0.88 ± 0.21 (tumor/blood), and 7.3 ± 3.5 (tumor/other tissue).

Juweid et al. (15) studied the feasibility of ^131^I-NP-4 F(ab´)_2_ for use in therapy in 13 cancer patients (8 colorectal, 3 lung, 1 pancreatic, and 1 medullary thyroid cancer). The mean plasma CEA level was 120 ng/ml with 11 patients having ≤100 ng/ml. The radioactivity dose was based on a prescribed red marrow dose, which was determined by a tracer study dose, of 370-555 MBq (10-15 mCi). The average blood and total-body t_½_ values in the 12 patients with a human anti-mouse antibody (HAMA) level <100 ng/ml were 15.3 ± 4.7 and 49.5 ± 13.1 h, respectively. Dosimetry studies showed that the absorbed doses (cGy/mCi) were 0.5 ± 0.1 (whole body), 1.8 ± 0.4 (red marrow), 3.3 ± 1.9 (kidneys), 1.6 ± 0.7 (liver), 2.1 ± 0.6 (lung), and 4.4 ± 2.7 (spleen).

Goldenberg et al. (14) evaluated colorectal cancer imaging with ^123^I-NP-4 F(ab´)_2_ in a prospective, randomized multicenter study of 58 patients. Patients received doses of 296-370 MBq (8-10 mCi) in1 or 10 mg of either ^123^I-NP-4 F(ab´)_2_ or ^123^I-NP-4 Fab´. Imaging was performed at 2-4, 24, and 48 h after antibody administration. Of the 58 patients, 17 received 1 mg and 14 received 10 mg of ^123^I-NP-4 F(ab´)_2._ For ^123^I-NP-4 Fab´, 12 patients received 1 mg and 15 patients received 10 mg. The median biological blood t_½α_ and t_½β_ values for ^123^I-NP-4 F(ab´)_2_ were 1.6 and 26 h, respectively. For ^123^I-NP-4 Fab´, these values were 2.4 and 19 h, respectively. No difference was observed between the imaging results of the 4 groups. No dose dependence for the antibody targeting was found. There appeared to be no correlation between sensitivity and size of lesions or serum CEA level. Single-photon emission computed tomography (SPECT) evaluation was judged to be more beneficial than planar imaging in 47% of the cases. Sensitivity, specificity, and accuracy for all regions and all four arms of the studies were 86, 89, and 89%, respectively. The positive predictive value by tumor lesions was 91%. Only one patient developed a low level of HAMA.

## NIH Support

NCI CA39841,

## References

1 Behr T.M., Sharkey R.M., Juweid M.E., Dunn R.M., Vagg R.C., Ying Z., Zhang C.H., Swayne L.C., Vardi Y., Siegel J.A., Goldenberg D.M. (1997). Phase I/II clinical radioimmunotherapy with an iodine-131-labeled anti-carcinoembryonic antigen murine monoclonal antibody IgG. J Nucl Med.
2 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
3 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
4 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
5 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
6 (1999). . CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab, Immunomedics, Inc. p. 1-15.
7 Sharkey R.M., Goldenberg D.M., Goldenberg H., Lee R.E., Ballance C., Pawlyk D., Varga D., Hansen H.J. (1990). Murine monoclonal antibodies against carcinoembryonic antigen: immunological, pharmacokinetic, and targeting properties in humans. Cancer Res.
8 Covell D.G., Barbet J., Holton O.D., Black C.D., Parker R.J., Weinstein J.N. (1986). Pharmacokinetics of monoclonal immunoglobulin G1, F(ab')2, and Fab' in mice. Cancer Res.
9 Behr T.M., Goldenberg D.M., Scheele J.R., Wolf F.G., Becker W. (1997). Clinical relevance of immunoscintigraphy with 99mTc-labelled anti-CEA antigen-binding fragments in the follow-up of patients with colorectal carcinoma. Assessment of surgical resectability with a combination of conventional imaging methods. Dtsch Med Wochenschr.
10 Sharkey R.M., Primus F.J., Shochat D., Goldenberg D. M. (1988). Comparison of tumor targeting of mouse monoclonal and goat polyclonal antibodies to carcinoembryonic antigen in the GW-39 human tumor-hamster host model. Cancer Research.
11 Sharkey R.M. Gold D.V. Aninipot R. Vagg R. Ballance C. Newman E.S. Ostella F. Hansen H.J. Goldenberg D.M. Comparison of tumor targeting in nude mice by murine monoclonal antibodies directed against different human colorectal cancer antigens Cancer Res 1990 50Suppl3 828s 834s 2297729
12 Sharkey R.M., Motta-Hennessy C., Pawlyk D., Siegel J.A., Goldenberg D.M. (1990). Biodistribution and radiation dose estimates for yttrium- and iodine-labeled monoclonal antibody IgG and fragments in nude mice bearing human colonic tumor xenografts. Cancer Res.
13 Blumenthal R.D., Sharkey R.M., Kashi R., Goldenberg D.M. (1989). Comparison of therapeutic efficacy and host toxicity of two different 131I-labelled antibodies and their fragments in the GW-39 colonic cancer xenograft model. Int J Cancer.
14 Goldenberg D.M., Wlodkowski T.J., Sharkey R.M., Silberstein E.B., Serafini A.N., Garty II, Van Heertum R.L., Higginbotham-Ford E.A., Kotler J.A., Balasubramanian N. (1993). Colorectal cancer imaging with iodine-123-labeled CEA monoclonal antibody fragments. J Nucl Med.
15 Juweid M.E., Sharkey R.M., Behr T., Swayne L.C., Dunn R., Siegel J., Goldenberg D.M. (1996). Radioimmunotherapy of patients with small-volume tumors using iodine-131-labeled anti-CEA monoclonal antibody NP-4 F(ab')2. J Nucl Med.
16 Blumenthal R.D., Sharkey R.M., Haywood L., Natale A.M., Wong G.Y., Siegel J.A., Kennel S.J., Goldenberg D.M. (1992). Targeted therapy of athymic mice bearing GW-39 human colonic cancer micrometastases with 131I-labeled monoclonal antibodies. Cancer Res.
17 Fand I., Sharkey R.M., Grundy J.P., Goldenberg D.M. (1992). Localization by whole-body autoradiography of intact and fragmented radiolabeled antibodies in a metastatic human colonic cancer model. Int J Rad Appl Instrum B.
18 Murray J.L. Rosenblum M.G. Zhang H.Z. Podoloff D.A. Kasi L.P. Curley S.A. Chan J.C. Roh M. Hohn D.C. Brewer H. Cunningham J.E. Thompson L.B. Bhadkamkar M.S. Pinsky C.M. Fogler W.E. Comparative tumor localization of whole immunoglobulin G anticarcinoembryonic antigen monoclonal antibodies IMMU-4 and IMMU-4 F(ab')2 in colorectal cancer patients Cancer 1994 73Suppl3 850 7 8306270